# O-(3-[^18^F]Fluoropropyl)-L-tyrosine

Chemical name: | O-(3-[^18^F]Fluoropropyl)-L-tyrosine
Abbreviated name: | FPT, [^18^F]FPT
Synonym:
Agent category: | Compound
Target: | L-type amino acid transporter system and Na^+^-dependent system B^0^
Target category: | Transporter
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22O-%283-fluoropropyl%29tyrosine%22%5BSubstance%20Name%5D)]

A variety of [^11^C] and [^18^F] labeled amino acids have been studied for potential use in positron emission tomography (PET) oncology (1, 2). Most brain tumors show an increased uptake of amino acids as compared with normal brain (3). These amino acids are composed of naturally occurring amino acids such as, L-[^11^C]leucine, L-[^11^C]methionine (MET), and L-[^11^C]tyrosine and non-natural amino acids such as [^11^C]aminoisobutyric acid, [^11^C]1-aminocyclopentane-1-carboxylic acid, and [^11^C]1-aminocyclobutane-1-carboxylic acid. There are also ^123^I-labeled amino acids used in imaging in oncology (1, 4, 5).

Some 20 amino acid transporter systems have been identified (1). Most of the amino acids are taken up by tumor cells through an energy-independent L-type amino acid transporter system and a sodium-dependent transporter system A but also a Na^+^-dependent system B^0^ (6). They are retained in tumor cells due to their higher metabolic activities including incorporation into proteins than most normal cells (1). Malignant transformation increases the use of amino acids for energy, protein synthesis and cell division. Tumor cells were found to have over-expressed transporter systems (7). L-[^11^C]MET, [^18^F]fluorotyrosine, L-[^11^C]leucine, and [^18^F]fluoro-α-methyl tyrosine have been widely used in detection of tumors (2, 6) but are not approved by the FDA. They are moved into cells by various amino acid transporters and are incorporated into proteins. The fraction of radiolabeled amino acid that is incorporated into protein is usually small compared to the total amount taken up into the cell. These natural amino acid images are based on amino acid transport and protein incorporation.

All of the non-natural amino acids are not incorporated into proteins (2, 8). These amino acids are rapidly transported into cells. Recently, a new L-tyrosine analog, O-(3-[^18^F]Fluoropropyl)-L-tyrosine (FPT), was synthesized and evaluated as an amino acid PET tracer for detection of tumors with a higher specificity as compared to FDG (9-11). Therefore, FPT could be a promising tracer in PET tumor imaging based solely on amino acid transport.

### Related Resource Links:

- Chapters in MICAD (Amino acid transporters (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=amino%20acid%20(transporter%20OR%20transporters)+AND+micad%5Bbook%5D))
- Gene information in NCBI (L-type amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/23428), A-type amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/54407))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Amino acid transporters (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=amino%5BAll+Fields%5D+AND+acid%5BAll+Fields%5D+AND+transporter%5BAll+Fields%5D))
- Clinical trials (Amino acid transporters (http://www.clinicaltrials.gov/ct2/results?term=amino+acid+transporters))
- Drug information in FDA (Amino acid transporters (http://google2.fda.gov/search?q=amino+acid+transporters&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22O-%283-fluoropropyl%29tyrosine%22%5BSubstance%20Name%5D%20AND%20synthesis%5BAll%20Fields%5D)]

FPT was prepared by [^18^F]fluoropropylation of L-tyrosine in a two-step procedure (9). [^18^F] fluorination (K[^18^F]F/Kryptofix 2.2.2.) of 1,3-ditosyloxypropane led to a yield of 40-50% with no decay correction. The radiochemical purity of 1-[^18^F]fluoro-3-tosyloxypropane was about 100%. Subsequently, fluoropropylation with unprotected L-tyrosine by 1-[^18^F]fluoro-3-tosyloxypropane were performed to give FPT in 60% yield with a chemical purity of >95%. The overall radiochemical yield was about 25-30% in 60 min. This method was automated to give a radiochemical yield of 12% (not decay corrected) in 52 min and a radiochemical purity of >95% (10)

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22O-%283-fluoropropyl%29tyrosine%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

O-(2-[^18^F]Fluoroethyl)-L-tyrosine (FET), a close analog to FPT, was shown to be transported mainly (80%) by the L-type amino acid transporter system and not incorporated into proteins in human SW 707 colon carcinoma cells (12). FET was also found to be transported into F98 rat gliomas (30%) by the Na^+^-dependent system B^0^ (6).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22O-%283-fluoropropyl%29tyrosine%22%5BSubstance%20Name%5D%20AND%20rodentia)]

Biodistribution of FPT was determined in normal mice with FPT, FET, and [^18^F]fluoro-2-deoxy-2-D-glucose (FDG) uptake studies in mice bearing S18 fibrosarcoma and Staphylococcus aureus-inoculated mice (9). Mice were injected with 0.74-1.48 MBq (20-40 μCi) of the tracers. In addition, S18-bearing mice and S. aureus-inoculated mice were imaged using FPT PET compared with FET and FDG PET imaging. High uptake and long retention time of FPT and FET in most organs, such as kidneys, liver, lung, blood, and heart, and low uptake in brain were found. Furthermore, high FPT, FET, and FDG uptake in tumor, and almost no FPT and FET uptake in inflammatory tissue, were observed. In contrast, FDG uptake in inflammatory tissue was high. FPT seems to be a potential amino acid tracer similar to FET for tumor imaging with PET.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22O-%283-fluoropropyl%29tyrosine%22%5BSubstance%20Name%5D%20and%20%28pig%20or%20dog%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22O-%283-fluoropropyl%29tyrosine%22%5BSubstance%20Name%5D%20AND%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22O-%283-fluoropropyl%29tyrosine%22%5BSubstance%20Name%5D%20and%20human)]

Internal dosimetry data for FPT in humans have not yet been available in the literature. The human dosimetry resulting from the intravenous administration of FPT were estimated using biodistribution data from normal mice (11). The highest uptake of FPT was found in the urinary bladder and pancreas, followed by the liver and kidneys. The urinary bladder wall received the highest absorbed dose of 101.0 μGy/MBq (373.7 mrad/mCi) for a 70-kg standard man. The brain received the lowest dose, 6.5 μGy/MBq or 24.1 mrad/mCi. Other organs received doses in the range of 6.5–37.5 μGy/MBq (24.1-138.8 mrad/mCi). The effective dose was 18.2 μSv/MBq (67.3 mrem/mCi). The data show that a 370-MBq (10 mCi) injection of FPT would lead to an estimated effective dose of 6.7 mSv (24.8 rem), which is in the accepted range of routine nuclear medicine investigations.

## References

1 Jager P.L., Vaalburg W., Pruim J., de Vries E.G., Langen K.J., Piers D.A. (2001). Radiolabeled amino acids: basic aspects and clinical applications in oncology. J Nucl Med.
2 Laverman P., Boerman O.C., Corstens F.H., Oyen W.J. (2002). Fluorinated amino acids for tumour imaging with positron emission tomography. Eur J Nucl Med Mol Imaging.
3 Herholz K., Heiss W.D. (2004). Positron emission tomography in clinical neurology. Mol Imaging Biol.
4 Langen K.J., Pauleit D., Coenen H.H. (2002). 3-[(123)I]Iodo-alpha-methyl-L-tyrosine: uptake mechanisms and clinical applications. Nucl Med Biol.
5 Lahoutte T., Caveliers V., Camargo S.M., Franca R., Ramadan T., Veljkovic E., Mertens J., Bossuyt A., Verrey F. (2004). SPECT and PET amino acid tracer influx via system L (h4F2hc-hLAT1) and its transstimulation. J Nucl Med.
6 Langen K.J., Jarosch M., Muhlensiepen H., Hamacher K., Broer S., Jansen P., Zilles K., Coenen H.H. (2003). Comparison of fluorotyrosines and methionine uptake in F98 rat gliomas. Nucl Med Biol.
7 Saier M.H., Daniels G.A., Boerner P., Lin J. (1988). Neutral amino acid transport systems in animal cells: potential targets of oncogene action and regulators of cellular growth. J Membr Biol.
8 Wester H.J., Herz M., Weber W., Heiss P., Senekowitsch-Schmidtke R., Schwaiger M., Stocklin G. (1999). Synthesis and radiopharmacology of O-(2-[18F]fluoroethyl)-L-tyrosine for tumor imaging. J Nucl Med.
9 Tang G., Wang M., Tang X., Luo L., Gan M. (2003). Synthesis and evaluation of O-(3-[18F]fluoropropyl)-L-tyrosine as an oncologic PET tracer. Nucl Med Biol.
10 Tang G., Tang X., Wang M., Luo L., Gan M. (2003). Fully automated synthesis of O-(3-[18F]fluoropropyl)-L-tyrosine by direct nucleophilic exchange on a quaternary 4-aminopyridinium resin. Appl Radiat Isot.
11 Tang G., Tang X., Wang M., Luo L., Gan M. (2004). Radiation dosimetry of O-(3-[18F]fluoropropyl)-L-tyrosine as oncologic PET tracer based on the mice distribution data. Appl Radiat Isot.
12 Heiss P., Mayer S., Herz M., Wester H.J., Schwaiger M., Senekowitsch-Schmidtke R. (1999). Investigation of transport mechanism and uptake kinetics of O-(2-[18F]fluoroethyl)-L-tyrosine in vitro and in vivo. J Nucl Med.